# 2-(4'-Dimethylaminophenyl)-6-[^125^I]iodobenzothiazole

Chemical name: | 2-(4'-Dimethylaminophenyl)-6-[^125^I]iodobenzothiazole
Abbreviated name: | [^125^I]TZDM
Synonym:
Agent Category: | Compound
Target: | Amyloid β (Aβ) aggregates
Target Category: | Binding
Method of detection: | SPECT
Source of signal: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28125I%29TZDM)]

Alzheimer’s disease (AD) is a major neurodegenerative disease associated with an irreversible decline of mental functions and with cognitive impairment (1). It is characterized by the presence in the brain of senile plaques of β-amyloid (Aβ) peptides with intracellular neurofibrillary tangles of filaments that contain the hyperphosphorylated protein tau (2, 3). Accelerated deposition of Aβ deposits seems to be a key risk factor associated with AD, and although the mechanisms of the disease are still not fully understood, reducing the deposition of amyloid plaques seems to benefit patients.

Several radioligands have been developed (4-6) and tested in humans as in vivo diagnostic tools for imaging and measuring the formation of Aβ deposits (6). The first agent successfully used in human studies was [^18^F]FDDNP (7), a malonitrile derivative found to bind to both neurofibrillary tangles and Aβ plaques. The second successful attempt was made with [^11^C]PIB (8), also known as Pittsburgh Compound B or [^11^C]6-OH-BTA-1, which showed marked retention in areas of the cortex known to contain substantial amounts of Aβ deposits. The third PET radioligand successfully tested in humans was [^11^C]4-N-methylamino-4´-hydroxystilbene, a stilbene derivative commonly named [^11^C]SB-13 that exhibited good binding affinities for Aβ aggregates in vitro, moderate lipophilicity, high initial brain uptake in the normal rat cortex, and a rapid washout (9).

Benzofuran derivatives labeled with radioactive iodine have shown very good binding affinities for Aβ aggregates and good brain penetration (10). Unfortunately, their level of nonspecific binding was found to be very high, which makes them unsuitable for in vivo plaque imaging. However, [^125^I]IMPY displayed good initial brain uptake and rapid washout from normal mouse brain and postmortem AD brain sections (11). Several conjugated thioflavin compounds based on benzothiazole have been shown to bind specifically to amyloid plaques. However, the thioflavins contain an ionic quaternary amine that is permanently charged and unfavorable to brain uptake. For that reason, several alternatives that use neutral derivatives have been synthesized and are currently being evaluated as potential ligands for imaging Aβ deposits in the AD brain. One of them, 2-(4'-dimethylaminophenyl)-6-[^125^I]iodobenzothiazole ([^125^I]TZDM) is currently being studied both in vitro and in vivo (12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28125I%29TZDM%20AND%20synthesis)]

[^125^I]TZDM was prepared by Zhuang et al. (12) using a iododestannylation reaction with the tributyltin precursor 2-[4'-(dimethylamino)phenyl]-6-(tributylstannyl)benzothiazole. Briefly, hydrogen peroxide was added to a mixture of the tributyltin precursor (1 mg/ml EtOH), HCl, and Na^125^I [ 0.037–0.185 MBq (1–5 µCi)] in a closed vial. The reaction was allowed to proceed at room temperature for 10 min and was ended by the addition of saturated NaHSO_3_. The reaction mixture was then extracted after neutralization with a saturated sodium bicarbonate solution. After purification on a C4 column eluted with an isocratic solvent of 80% acetonitrile and 20% 3,3-dimethylglutaric acid (pH 7.0) at a flow rate of 0.8 ml/min, the desired fractions containing the product were collected, condensed, and re-extracted with ethyl acetate.

The no-carrier-added products were evaporated to dryness and redissolved in 100% EtOH. This reaction produced a no-carrier-added tracer with a specific activity comparable to that of Na^125^I [ 59.4 MBq/mmol (2,200 Ci/mmol)] at the end of reaction. [^125^I]TZDM was found to be stable in vitro for up to 2 months (storage at -20ºC), with a radiochemical purity >95% as determined by high-performance liquid chromatography (12).

The precursor was prepared from a solution of 2-[4'-(dimethylamino)phenyl]-6-bromobenzothiazole (60 mg, 0.18 mmol) in 1,4-dioxane (2 ml), toluene (2 ml), and triethylamine (2 ml) with successive additions of (Bu_3_Sn)_2_ and Pd(Ph_3_P)_4_. After stirring at 90ºC overnight, the solvent was removed and the residue purified by preparative thin-layer liquid chromatography (12).

## In Vitro Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28125I%29TZDM%20AND%20in%20vitro)]

Zhuang et al. (12) performed in vitro binding assays of [^125^I]TZDM to Aβ aggregates using Aβ(1–40) and Aβ(1–42) peptides in solution. Results showed that the ligand displayed a saturable binding, probably with one-site binding (as suggested by the linearity of the transformation of the saturation binding to Scatchard plots) and a preference for Aβ(1–42) aggregates. The estimated dissociation constants reported by Zhuang et al. (12) were 0.06 nM for aggregates of Aβ(1–40) and 0.14 nM for Aβ(1–42) aggregates.

Zhuang et al. (12) also performed competitive studies to evaluate the two styrylbenzene derivatives, chrysamine G and (E,E)-1-iodo-2,5-bis(3-hydroxycarbonyl-4-hydroxy)styrylbenzene (IMSB), versus [^125^I]TZDM with respect to binding properties on Aβ (1–40) and Aβ (1–42) aggregates. High inhibition constants (K_i_) were observed, which indicated poor binding competition. Similarly, high K_i_ values were obtained for [^125^I]TZDM compared with binding of [^125^I]IMSB [K_i_ (25ºC) >2000 for Aβ(1–40) and K_i_ (25ºC) >2000 for Aβ(1–40)]. The reported K_i_ values for TZDM versus [^125^I]TZDM were 0.9 ± 0.2 for Aβ(1–40) and 2.2 ± 0.4 for Aβ(1–42). Three sets of experiments were performed, each carried out in duplicate.

The observations and results reported by Zhuang et al. (12) highlighted that fact that [^125^I]TZDM displayed distinctive and mutually exclusive binding sites for Aβ(1–40) and Aβ(1–42) aggregates. Because increased production and deposition of Aβ(1–42) relative to Aβ(1–40) may be crucial for the generation of senile plaques, [^125^I]TZDM and other related derivatives may be attractive imaging probes for in vivo plaque labeling. Zhuang et al. (12) pointed out the need for additional studies to provide further insight into structural information of the potential binding sites and the extent of functional linkages of benzothiazole binding sites on Aβ aggregates.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28125I%29TZDM%20AND%20rodentia%5BmeSH%5D)]

To test the permeability of [^125^I]TZDM through the intact blood–brain barrier, Zhaung et al. (12) injected 0.18–0.37 MBq (5–10 µCi) of the radioligand into the tail vein of normal mice (2–3 months old, 20–30 g each). The mice were euthanized at various times after injection, the organs of interest were excised and weighed, and their radioactivity was measured. Brain uptake results (in % dose/organ, average of 3 or 4 mice) were: 0.6 ± 0.11 (at 2 min postinjection), 0.9 ± 0.29 (30 min), 1.57 ± 0.24 (60 min), 0.65 ± 0.11 (6 h), and 0.04 ± 0.01 (24 h). Brain uptake peaked at 60 min, and blood levels were relatively low throughout the evaluated time period. Radioactivity uptake values (in % dose/organ) for other organs of interest included 0.6 ± 0.11 (at 2 min postinjection), 0.9 ± 0.29 (30 min), 1.57 ± 0.24 (60 min), 0.65 ± 0.11 (6 h), and 0.04 ± 0.01 (24 h) for the kidney; 0.6 ± 0.11 (at 2 min postinjection), 0.9 ± 0.29 (30 min), 1.57 ± 0.24 (60 min), 0.65 ± 0.11 (6 h), and 0.04 ± 0.01 (24 h) for the liver; 0.6 ± 0.11 (at 2 min postinjection), 0.9 ± 0.29 (30 min), 1.57 ± 0.24 (60 min), 0.65 ± 0.11 (6 h), and 0.04 ± 0.01 (24 h) for the heart.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28125I%29TZDM%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28125I%29TZDM%20AND%20%28%28primate%20NOT%20human%29%20OR%20baboon%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28125I%29TZDM%20AND%20human)]

No publication is currently available.

## References

1 Forstl H., A. Kurz. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
3 Brandt R., J. Leschik. (2004). Functional interactions of tau and their relevance for Alzheimer's disease. Curr Alzheimer Res.
4 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
5 Bacskai B.J., G.A. Hickey, J. Skoch, S.T. Kajdasz, Y. Wang, G.F. Huang, C.A. Mathis, W.E. Klunk, B.T. Hyman. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
6 Wu C., V.W. Pike, Y. Wang. (2005). Amyloid imaging: from benchtop to bedside. Curr Top Dev Biol.
7 Shoghi-Jadid K., G.W. Small, E.D. Agdeppa, V. Kepe, L.M. Ercoli, P. Siddarth, S. Read, N. Satyamurthy, A. Petric, S.C. Huang, J.R. Barrio. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
8 Klunk W.E., H. Engler, A. Nordberg, Y. Wang, G. Blomqvist, D.P. Holt, M. Bergstrom, I. Savitcheva, G.F. Huang, S. Estrada, B. Ausen, M.L. Debnath, J. Barletta, J.C. Price, J. Sandell, B.J. Lopresti, A. Wall, P. Koivisto, G. Antoni, C.A. Mathis, B. Langstrom. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
9 Ono M., A. Wilson, J. Nobrega, D. Westaway, P. Verhoeff, Z.P. Zhuang, M.P. Kung, H.F. Kung. (2003). 11C-labeled stilbene derivatives as Abeta-aggregate-specific PET imaging agents for Alzheimer's disease. Nucl Med Biol.
10 Ono M., M.P. Kung, C. Hou, H.F. Kung. (2002). Benzofuran derivatives as Abeta-aggregate-specific imaging agents for Alzheimer's disease. Nucl Med Biol.
11 Kung M.P., C. Hou, Z.P. Zhuang, B. Zhang, D. Skovronsky, J.Q. Trojanowski, V.M. Lee, H.F. Kung. (2002). IMPY: an improved thioflavin-T derivative for in vivo labeling of beta-amyloid plaques. Brain Res.
12 Zhuang Z.P., M.P. Kung, C. Hou, D.M. Skovronsky, T.L. Gur, K. Plossl, J.Q. Trojanowski, V.M. Lee, H.F. Kung. (2001). Radioiodinated styrylbenzenes and thioflavins as probes for amyloid aggregates. J Med Chem.